# ^64^Cu-Labeled DOTA-conjugated rituximab, a chimeric murine/human anti-CD20 monoclonal antibody

Chemical name: | ^64^Cu-Labeled DOTA-conjugated rituximab, a chimeric murine/human anti-CD20 monoclonal antibody
Abbreviated name: | [^64^Cu]-DOTA-Rituximab
Synonym: | MabThera^®^; Rituxan^®^
Agent Category: | Antibody
Target: | Cell differentiation antigen 20 (CD20)
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=rituximab&cmd=DetailsSearch)]

Rituximab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=b172773b-3905-4a1c-ad95-bab4b6126563) is a chimeric murine/human monoclonal antibody (mAb) that targets the CD20 antigen (also known as membrane-spanning 4-domains, subfamily A, member 1, or MS4A1) and has been approved by the United States Food and Drug Administration for the treatment of non-Hodgkins lymphomas (http://cancer.gov/cancertopics/types/non-hodgkin) (NHL; diffused large-B cell, low-grade, or follicular types), rheumatoid arthritis (http://www.nlm.nih.gov/medlineplus/rheumatoidarthritis.html), granulomatosis with polyangiitis (http://www.rheumatology.org/practice/clinical/patients/diseases_and_conditions/wegeners.asp) (Wegener's granulomatosis) and microscopic polyangiitis (http://rarediseases.info.nih.gov/GARD/Condition/3652/Microscopic_polyangiitis.aspx). The exact mechanism of action of rituximab has been discussed by Maloney (1). Although much is known about the pathogenesis of the different forms of NHL at the molecular level, the prognosis for an individual suffering from this disease is based on the morphological and histological information obtained with invasive methods used on the patients (2). Therefore, the use of noninvasive procedures, such as imaging with radiolabeled agents, is an attractive option to screen for patients who can benefit the most from an anti-cancer treatment, and the same imaging technique(s) can be used to monitor and assess the efficacy of a treatment (3). In the clinic, positron emission tomography (PET) is commonly used to detect, stage, and monitor the treatment outcome for various cancers because this imaging modality has superior penetration and sensitivity and it is more quantitative compared with other imaging techniques such as single-photon emission computed tomography, magnetic resonance imaging, ultrasound, and optical imaging (4). In this regard, there is much effort devoted to the development of radiolabeled mAbs that can be used with PET for the targeted imaging of neoplasms that express specific antigens, such as the epidermal growth factor receptor (5) and the carcinoembryonic antigen (6).

^64^Cu-Labeled rituximab ([^64^Cu]-DOTA-rituximab) was developed in an effort to generate a PET imaging agent that can be used to monitor the treatment of NHL (2). The biodistribution of [^64^Cu]-DOTA-rituximab was studied with PET in huCD20 transgenic mice, which mimic the human B-cell lymphoma tumors (obtained from Genentech Corporation, CA) (2).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Rituximab+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human CD20 protein (http://www.ncbi.nlm.nih.gov/protein/NP_068769.2) and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_152866.2) (MS4A1 transcript variant 1) sequences

Human CD20 in Gene database (http://www.ncbi.nlm.nih.gov/gene/931); Gene ID: 931

Information on human CD20 in Online Mendelian Inheritance in Man database (OMIM (http://omim.org/entry/112210))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=CD20&Search=Search) regarding CD20

Rituximab-related clinical trials (http://clinicaltrials.gov/ct2/results?term=Rituximab&Search=Search)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-DOTA-rituximab%20synthesis&cmd=DetailsSearch)]

Rituximab was purchased from a commercial source and conjugated to 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) to form DOTA-rituximab for the chelation of ^64^Cu ([^64^Cu]-DOTA-rituximab) as described by Natarajan et al. (2). The labeled mAb was purified with size-exclusion chromatography, formulated in phosphate-buffered saline (pH 7.4), and filtered through a 0.22-micron filter for storage in a sterile vial (storage conditions not described). Matrix-assisted laser desorption/ionization-time of flight analysis of the DOTA-rituximab preparation showed that 1–2 DOTA molecules were conjugated with each molecule of rituximab. The radiochemical yield (RCY) of the labeling reaction was reported to be 70%–80%, and the radiochemical purity (RCP) of the final preparation was >95%. The specific activity of [^64^Cu]-DOTA-rituximab was 3.7–4.7 MBq/6.7 pmol (136.9–173.9 μCi/6.7 pmol) (2).

The radiolabeled mAb was stable in human serum at 37°C for at least 3 days (>98% remained intact), as determined with cellulose acetate electrophoresis (2).

The synthesis of [^64^Cu]-DOTA-rituximab was also reported by Jalilian et al. (7). The mAb was obtained from a commercial source and labeled with ^64^Cu as described elsewhere (7). The RCY and the RCP of the labeled mAb were 82% and 90%–95%, respectively, and the specific activity of [^64^Cu]-DOTA-rituximab was reported to be 30 GBq/6.7 nmol (1.11 Ci/6.7 nmol). The ^64^Cu-labeled mAb was reported to be stable in human serum at 37°C for at least 24 h, as determined with thin-layer chromatography.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22231277%5Buid%5D&cmd=DetailsSearch)]

The immunoreactivity of [^64^Cu]-DOTA-rituximab was studied in cell binding assays with two CD20^+^ cell lines (Ramos cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1596&Template=cellBiology) and Daudi cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-213&Template=cellBiology)) and a CD20^–^ cell line (Jurkat cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=TIB-152&Template=cellBiology); used as a negative control) (2). Binding assays were performed with two sets of each cell line: the first set of cells was blocked with nonradiolabeled rituximab (0.13 pmol or 0.67 pmol) 2 h prior to the addition of [^64^Cu]-DOTA-rituximab (0.065 pmol and 0.013 pmol, respectively, per assay tube), and the second set of cells was exposed to the radiolabeled mAb without prior blocking of the antigen. The different cell suspensions were incubated with the tracer at 37°C for 2 h, and the amount of radioactivity bound to the cells was determined as described elsewhere (2). Approximately 80% of the added radioactivity was bound to the unblocked Ramos cells and Daudi cells, whereas the Jurkat cells showed a binding of only 6% of the total added tracer. Ramos cells and Daudi cells exposed to a blocking dose of rituximab bound only ~3% of the added probe, and this amount of label was similar to that detected on the Jurkat cells under the same conditions. These results indicated that the binding specificity of [^64^Cu]-DOTA-rituximab to the CD20 antigen was not altered either by the conjugation of DOTA to rituximab or by the chelation of ^64^Cu to DOTA-rituximab.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-DOTA-rituximab%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^64^Cu]-DOTA-rituximab was studied in two groups of human CD20^+^ transgenic mice (n = 6 animals/group) as described elsewhere (2). One group of mice received a blocking dose of nonradioactive rituximab (13.5 nmol/kg body weight) through the tail vein 2 h before the labeled mAb (7.4 MBq/13.5 pmol (200 μCi/13.5 pmol)) was administered to the animals through the same route. The second group of animals did not receive a blocking dose of the mAb and were injected with the probe as described above. PET images were acquired from both groups of animals at various time points ranging from 4 h to 48 h postinjection (p.i.). From the images it was evident that the label was present primarily in the spleen and liver of the unblocked animals, even at 24 h p.i. By 48 h p.i., all radioactivity had cleared from the liver, but some label was present in the spleen of these animals (probably because the spleen contains a high number of lymphocytes that express the CD20 antigen on the cell surface). The amount of radioactivity in the spleen of the unblocked and blocked animals (time point not mentioned) was 16.5 ± 0.45% injected dose per gram tissue (% ID/g) and 1.76 ± 0.43% ID/g, respectively. The amount of tracer in the liver of unblocked and blocked animals was 0.52 ± 0.17% ID/g and 0.41 ± 0.51% ID/g, respectively, at the same time point.

From these studies, the investigators concluded that [^64^Cu]-DOTA-rituximab can be a suitable imaging agent to monitor the treatment of NHL in rodents (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-DOTA-rituximab%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-DOTA-rituximab%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies reported in this chapter were supported in part by a National Cancer Institute In Vivo Cellular and Molecular Imaging Centers grant P50-CA114747.

## References

1 Maloney D.G. (2012). Anti-CD20 antibody therapy for B-cell lymphomas. N Engl J Med.
2 Natarajan A., Gowrishankar G., Nielsen C.H., Wang S., Iagaru A., Goris M.L., Gambhir S.S. (2012). Positron Emission Tomography of (64)Cu-DOTA-Rituximab in a Transgenic Mouse Model Expressing Human CD20 for Clinical Translation to Image NHL. Mol Imaging Biol.
3 Willmann J.K., van Bruggen N., Dinkelborg L.M., Gambhir S.S. (2008). Molecular imaging in drug development. Nat Rev Drug Discov.
4 Kobayashi H., Longmire M.R., Ogawa M., Choyke P.L. (2011). Rational chemical design of the next generation of molecular imaging probes based on physics and biology: mixing modalities, colors and signals. Chem Soc Rev.
5 Carlsson J. (2012). Potential for clinical radionuclide-based imaging and therapy of common cancers expressing EGFR-family receptors. Tumour Biol.
6 Wu A.M. (2009). Antibodies and antimatter: the resurgence of immuno-PET. J Nucl Med.
7 Jalilian A.R., Mirsadeghi L., Yari-kamrani Y., Rowshanfarzad P., Kamalidehghan M., Sabet M. (2007). Development of [64Cu]-DOTA-anti-CD20 for targeted therapy. Journal of Radioanalytical and Nuclear Chemistry.